# ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-regioselectively addressable functionalized template-[cyclo-(Arg-Gly-Asp-D-Phe-Lys)]_4_

Chemical name: | ^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-regioselectively addressable functionalized template-[cyclo-(Arg-Gly-Asp-D-Phe-Lys)]_4_ | [image]
Abbreviated name: | ^111^In-DOTA-RAFT-RGD | [image]
Synonym: | ^111^In-DOTA-RAFT-c(-RGDfK-)_4_ | [image]
Agent Category: | Peptides | [image]
Target: | Integrin α_v_β_3_ | [image]
Target Category: | Receptors | [image]
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging | [image]
Source of signal / contrast: | ^111^In | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of ^111^In-DOTA-RAFT-RGD (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=molecular%20imaging%20and%20integrin%20%CE%B1v%CE%B23)]

^111^In-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-regioselectively addressable functionalized template (RAFT)-[cyclo-(Arg-Gly-Asp-D-Phe-Lys)]_4_, abbreviated as ^111^In-DOTA-RAFT-RGD, is a tetrameric Arg-Gly-Asp (RGD)-based peptide conjugate synthesized by Ahmadi et al. for tumor imaging by targeting integrin α_v_β_3_ (1).

Angiogenesis is a process of neovascular development and growth from pre-existing vessels. Different from the normal blood vessel system, the neovasculature is chaotic and irregular in tumors with abnormal expression of diverse vascular surface biomarkers. These biomarkers have fewer kinetic compartments that must be crossed for intravenously administered agents to reach them (2, 3). Integrin α_v_β_3_ is one of these biomarkers and has been intensively investigated as a target for imaging and antiangiogenic therapy. Integrin α_v_β_3_ is minimally expressed in normal blood vessels but is significantly overexpressed in newly sprouting vasculature in tumors (4, 5). Small peptides are one group of ligands frequently used for targeting purposes, such as RGD, Asp-Gly-Arg, His-Gly-Phe, and Arg-Arg-Leu (3). The RGD tripeptide sequence is an adhesive protein recognition site, presenting in the extracellular matrix and blood. Integrin α_v_β_3_ binds extracellular matrix proteins through the exposed RGD tripeptide sequence. In general, RGD peptides are less selective (binding with 8 of the 24 integrins), degrade rapidly in vivo, and have a relatively low binding affinity (3, 6).

Development of multivalent RGD peptides is one approach to improve their properties. Boturyn et al. synthesized a RAFT-RGD platform based on a cyclic decapeptide scaffold that incorporates and presents in a spatially controlled manner two independent functional domains: a clustered ligand domain for integrin recognition and cell targeting, and a labeling domain for detection and characterization of this binding (7). This platform has been labeled with Cy5, ^99m^Tc, and ^64^Cu and has been shown to efficiently accumulate in tumors in animal models (8-11). Although the results are promising, approximately 30%–50% of the total dose of the labeled RAFT-RGD has been found to remain trapped in the kidneys several days after injection, which is at least partially due to the tetramerization of RGD peptides (1, 8, 12). Although peptides can be reabsorbed, endocytosed, and degraded by the lysosomes of proximal tubular cells, radiometal-chelated amino acids may be retained in the tubular cells, leading to radiation-induced toxicity and a weak imaging contrast for tumors surrounding the kidneys.

To reduce the renal accumulation of fluorescent and radiolabeled RAFT-RGD, Briat et al. evaluated the effect of Gelofusine on the renal reabsorption of these agents (13). Gelofusine is a gelatin-based plasma expander that consists of succinylated bovine gelatine molecules, a mixture of collagen-derived peptides. Infusion of Gelofusine has been reported to increase the renal excretion of megalin ligands and decrease the retention of radiolabeled compounds in the cortical proximal tubules (14-16). The results by Briat et al. showed that Gelofusine significantly reduced the renal retention of labeled RAFT-RGD, while it increased the ratio of tumor to healthy tissue (13). This chapter summarizes the data obtained with ^111^In-DOTA-RAFT-RGD and Gelofusine.

### Related Resource Links:

Integrin α_v_β_3_-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Integrin%20%CE%B1v%CE%B23%20%20AND%20micad%5bbook%5d)

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=integrin%20%CE%B1v%CE%B23) and protein (http://www.ncbi.nlm.nih.gov/protein?term=integrin%20%CE%B1v%CE%B23) sequences of integrin α_v_β_3_

Articles on integrin α_v_β_3_ (http://www.ncbi.nlm.nih.gov/omim?term=integrin%20%CE%B1v%CE%B23) in Online Mendelian Inheritance in Man

Integrin α_v_β_3_-related clinical trials (http://clinicaltrials.gov/ct2/results?term=integrin+%CE%B1v%CE%B23) in ClinicTrial.gov

Reference sequences of integrin members (http://www.ncbi.nlm.nih.gov/gene?term=integrin) in RefSeq

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=RAFT-RGD%20and%20imaging)]

Boturyn et al. described the three-step synthesis of DOTA-RAFT-RGD (7). Ahmadi et al. described the radiolabeling of DOTA-RAFT-RGD with [^111^In]InCl_3_ (1). The optimized labeling reaction was determined to be the addition of 55 MBq (1.49 mCi) [^111^In]InCl_3_ to 100 µg DOTA-RAFT-RGD in an ammonium acetate buffer (pH 4.8), heated for 30 min at 70°C for 30 min. DOTA-RAFT-RGD was labeled at a high radiochemical yield (> 97%) and purity (> 97%) in this condition (1). The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19111043)]

Ahmadi et al. analyzed the in vitro stability of ^111^In-DOTA-RAFT-RGD after incubation with human serum for 30 min to 24 h (1). ^111^In-DOTA-RAFT-RGD remained stable (95.6% intact) at 24 h, and only 2.5% of nonbound ^111^In was detected in human serum at 24 h, indicating a weak exchange reaction with plasma proteins and a high stability of the labeled complex.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=RAFT-RGD%20and%20imaging)]

Ahmadi et al. evaluated the in vivo metabolic stability of ^111^In-DOTA-RAFT-RGD in mice at 1, 4, and 24 h after injection of 2 MBq (0.054 mCi) of the tracer (n = 3 mice/time point, except 24 h, where n = 2) (1). Tissue homogenates were extracted, and the extraction efficiency for all tissues was between 77% and 99%. More than 90% of injected radioactivity was recovered from the purification column. Analysis of urine and liver extracts at 5 min and 25 min showed two peaks, which corresponded respectively to nonbound ^111^In and ^111^In-DOTA-RAFT-RGD. The radiochemical purity of ^111^In-DOTA-RAFT-RGD at 4 h after injection was 90% and 85% in the urine and liver, respectively. In the kidneys, 54.3% of the radioactivity corresponded to the intact tracer and ~25% to the nonbound ^111^In. Blood radioactivity was undetectable at 1 h after the tracer injection.

Ahmadi et al. further investigated the biodistribution of ^111^In-DOTA-RAFT-RGD in α_v_β_3_-positive TS/A-pc (murine mammary carcinoma cells) tumor-bearing mice (n = 8) (Table 1) (1). After injection of ^111^In-DOTA-RAFT-RGD (3.7 MBq (0.1 mCi)) through the tail vein, 15-min whole-body planar imaging was performed at 1, 4, 24, and 48 h, respectively. Animals were then euthanized. At 1 h after injection, ^111^In-DOTA-RAFT-RGD uptake in tumors was 1.63% injected dose per gram (ID/g), which decreased over time and stabilized between 24 h and 48 h. Clearance of the radioactivity from the blood circulation was fast, with the kidneys as the main route. Radioactivity in the kidneys was persistent with >30% ID/g. The tumor/blood and tumor/muscle ratios rapidly reached values above 1, and indicated that the imaging contrast was better at 24 h or 48 h after injection. Scintigraphic imaging confirmed these results and allowed the visualization of all tumors between 1 h and 48 h.

Table 1: Biodistribution data of ^111^In-DOTA-RAFT-RGD in TS/A-pc tumor-bearing mice.*

| Time after injection
Tissue (% ID/g) | 1 h | 4 h | 24 h | 48 h
Liver | 2.16 ± 0.81 | 1.30 ± 0.10 | 1.15 ± 0.08 | 1.29 ± 0.61
Kidney | 32.08 ± 14.59 | 52.73 ± 9.44 | 32.18 ± 1.58 | 32.69 ± 5.56
Blood | 2.77 ± 1.70 | 0.12 ± 0.05 | 0.03 ± 0.002 | 0.03 ± 0.01
Tumor | 1.63 ± 0.67 | 1.26 ± 0.18 | 0.77 ± 0.07 | 0.71 ± 0.17
Tumor/muscle | 2.67 | 9.69 | 4.35 | 5.13
Tumor/blood | 0.72 | 12.76 | 24.20 | 27.14

*Data were obtained by Ahmadi et al. (1).

Briat et al. studied the effect of Gelofusine on the biodistribution of ^111^In-DOTA-RAFT-RGD in mice bearing TS/A-pc tumors (n = 6 mice/group) (Table 2) (13). Each mouse received a tail vein injection of 12 MBq (0.32 mCi) ^111^In-DOTA-RAFT-RGD. Gelofusine (4%) or phosphate-buffered saline (PBS) was either pre-injected (5 min before tracer injection) or co-injected with the tracer. Similar to the data obtained by Ahmadi et al., ^111^In-DOTA-RAFT-RGD was primarily and rapidly cleared through the renal route. The amount of ^111^In-DOTA-RAFT-RGD was <1% ID/g in most organs at 1 h after injection except in the tumors and kidneys. Pre-injection and co-injection of Gelofusine strongly reduced the radioactivity in the kidneys by 49.2% and 47.9%, respectively (P = 0.002 and P < 0.0001). The radioactivity in the blood was comparable in the presence or absence of Gelofusine. Muscle uptake of ^111^In-DOTA-RAFT-RGD decreased by 10% in the presence of Gelofusine, whereas tumor uptake was not significantly affected (P > 0.05).

Briat et al. performed SPECT-CT imaging at 1 h and 24 h after injection of ^111^In-DOTA-RAFT-RGD (13). PBS or Gelofusine was pre-injected 5 min before the tracer (Table 2). Images showed that ^111^In-DOTA-RAFT-RGD was mainly localized in the renal cortex. In the presence of Gelofusine, this renal capture was also localized in the cortex but was greatly reduced. At 24 h after injection, the tracer uptake in the kidneys with Gelofusine preinjection was reduced by 49% and 66% as measured in the dissected kidneys and from the images, respectively, compared with PBS. The tumor/kidney but not the tumor/muscle ratio was significantly different between mice with PBS and those with Gelofusine injection (P < 0.05).

Table 2: Effect of Gelofusine on the biodistribution of ^111^In-DOTA-RAFT-RGD.

| PBS | | | Gelofusine
Ratio | 1 h | 24 h | Dissected* | 1 h | 24 h | Dissected*
Kidney | 13.35 ± 1.55 | 5.83 ± 0.52 | 42.30 ± 9.30 | 4.95 ± 0.95 | 1.97 ± 0.23 | 21.50 ± 9.30
T/M | 4.24 ± 0.44 | 4.50 ± 0.90 | 6.42 ± 2.30 | 3.63 ± 0.66 | 5.21 ± 0.76 | 7.03 ± 1.62
T/K | 0.06 ± 0.01 | 0.05 ± 0.01 | 0.03 ± 0.01 | 0.16 ± 0.02 | 0.16 ± 0.01 | 0.06 ± 0.01

*Data were obtained from dissected organs at 24 h after injection. Other data in the table were obtained directly from the images.

T/M = tumor/muscle ratio; T/K = tumor/kidney ratio.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Ahmadi M., Sancey L., Briat A., Riou L., Boturyn D., Dumy P., Fagret D., Ghezzi C., Vuillez J.P. (2008). Chemical and biological evaluations of an (111)in-labeled RGD-peptide targeting integrin alpha(V) beta(3) in a preclinical tumor model. Cancer Biother Radiopharm.
2 Cai W. (2008). andChen, X. Multimodality molecular imaging of tumor angiogenesis. J Nucl Med.
3 Lu X. (2012). andWang, R.F. A concise review of current radiopharmaceuticals in tumor angiogenesis imaging. Curr Pharm Des.
4 Beer A.J. (2008). andSchwaiger, M. Imaging of integrin alphavbeta3 expression. Cancer Metastasis Rev.
5 Gaertner, F.C.,Schwaiger, M., and Beer, A.J. Molecular imaging of avb3 expression in cancer patients. Q J Nucl Med Mol Imaging. 2010
6 Turkbey B., Kobayashi H., Ogawa M., Bernardo M., Choyke P.L. (2009). Imaging of tumor angiogenesis: functional or targeted?. AJR Am J Roentgenol.
7 Boturyn D., Coll J.L., Garanger E., Favrot M.C., Dumy P. (2004). Template assembled cyclopeptides as multimeric system for integrin targeting and endocytosis. J Am Chem Soc.
8 Jin Z.H., Josserand V., Razkin J., Garanger E., Boturyn D., Favrot M.C., Dumy P., Coll J.L. (2006). Noninvasive optical imaging of ovarian metastases using Cy5-labeled RAFT-c(-RGDfK-)4. Mol Imaging.
9 Jin Z.H., Josserand V., Foillard S., Boturyn D., Dumy P., Favrot M.C., Coll J.L. (2007). In vivo optical imaging of integrin alphaV-beta3 in mice using multivalent or monovalent cRGD targeting vectors. Mol Cancer.
10 Sancey L., Ardisson V., Riou L.M., Ahmadi M., Marti-Batlle D., Boturyn D., Dumy P., Fagret D., Ghezzi C., Vuillez J.P. (2007). In vivo imaging of tumour angiogenesis in mice with the alpha(v)beta (3) integrin-targeted tracer 99mTc-RAFT-RGD. Eur J Nucl Med Mol Imaging.
11 Garanger E., Boturyn D., Jin Z., Dumy P., Favrot M.C., Coll J.L. (2005). New multifunctional molecular conjugate vector for targeting, imaging, and therapy of tumors. Mol Ther.
12 Cheng, K.T.,Garanger, E.,Josserand, V.,Jin, Z.,Foillard, S.,Boturyn, D.,Favrot, P.M.C.,Dumy, P., and Coll, J.L. Cy5-Regioselectively addressable functionalized template-[cyclo-(RGD-d-Phe-Lys)]4 peptide. 2004
13 Briat A., Wenk C.H., Ahmadi M., Claron M., Boturyn D., Josserand V., Dumy P., Fagret D., Coll J.L., Ghezzi C., Sancey L., Vuillez J.P. (2012). Reduction of renal uptake of (111) In-DOTA-labeled and A700-labeled RAFT-RGD during integrin alpha(v) beta(3) targeting using single photon emission computed tomography and optical imaging. Cancer Sci.
14 Vegt E., Wetzels J.F., Russel F.G., Masereeuw R., Boerman O.C., van Eerd J.E., Corstens F.H., Oyen W.J. (2006). Renal uptake of radiolabeled octreotide in human subjects is efficiently inhibited by succinylated gelatin. J Nucl Med.
15 van Eerd J.E., Vegt E., Wetzels J.F., Russel F.G., Masereeuw R., Corstens F.H., Oyen W.J., Boerman O.C. (2006). Gelatin-based plasma expander effectively reduces renal uptake of 111In-octreotide in mice and rats. J Nucl Med.
16 ten Dam M.A., Branten A.J., Klasen I.S., Wetzels J.F. (2001). The gelatin-derived plasma substitute Gelofusine causes low-molecular-weight proteinuria by decreasing tubular protein reabsorption. J Crit Care.